# Cy5.5-Conjugated anti-epidermal growth factor receptor monoclonal antibody C225

Chemical name: | Cy5.5-Conjugated anti-epidermal growth factor receptor monoclonal antibody C225
Abbreviated name: | C225-Cy5.5
Synonym:
Agent Category: | Antibody
Target: | Epidermal growth factor receptor
Target Category: | Receptor
Method of detection: | Near-infrared fluorescence (NIR) imaging
Source of signal / contrast: | Cy5.5
Activation: | No
Studies: | - In vitro; - Non-primate non-rodent mammals | Click here for the protein and nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/6978796?ordinalpos=1&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) sequence of rat EGFR.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EGFR+Cy5%2E5)]

The epidermal growth factor receptor (EGFR) is often overexpressed or constitutively activated in several different cancer types, and these phenotypes are linked to an elevated metastatic potential, which indicates a poor prognosis for the patient (1-3). Because of its role in the development of cancer phenotypes, several anti-EGFR monoclonal antibodies (MAb), which are commercially available or under development and evaluation in clinical trials (http://clinicaltrials.gov/ct2/results?term=anti-EGFR+monoclonal+antibodies), have been approved by the United States Food and Drug Administration for the diagnosis and treatment of various cancers (4). It has also been shown that under preclinical (5, 6) and clinical (7) conditions, radioisotope-labeled anti-EGFR MAbs can be used for the diagnosis and treatment of cancers. In addition, as an alternative to the radiolabeled MAbs, anti-EGFR antibodies labeled with infrared fluorescent dyes have also been developed and evaluated in preclinical tumor xenograft models for the detection of cancers overexpressing EGFR, including oral cancer (8-11).

According to the Oral Cancer Foundation (http://www.oralcancerfoundation.org/facts/), >34,000 Americans will be diagnosed with oral or pharyngeal cancers this year, and among them ~8,000 will die from this condition. Oral cancer, ~90% of which is of the squamous cell carcinoma (SCC) type, is usually discovered at a late stage of development because it produces no pain and shows no symptoms during its early stages. Therefore, early detection of this cancer can result in the development of an appropriate, more aggressive, treatment regimen and increase the chances of a good prognosis. In an effort to produce a dual-purpose agent that could be used for early detection of oral cancer and also to determine the efficacy of an anti-cancer drug, Soukos et al. conjugated C225, an anti-EGFR MAb, to an infrared fluorescent dye, N,N’-di-carboxypentyl-indodicarbocyanine-5,5’-disulfonic acid (Cy5.5), and evaluated the conjugate for early detection of oral cancer in a hamster cheek pouch carcinogen evaluation model (11). The Cy5.5-conjugated MAb (C225-Cy5.5) was also used to monitor treatment of the cancer with chlorin_e6_ (C_e6_), a photosensitizer (http://www.cancer.gov/templates/db_alpha.aspx?CdrID=45836), conjugated to C225 (C225-C_e6_), which was used for photodynamic therapy (http://www.cancer.gov/Templates/db_alpha.aspx?CdrID=45238) of oral cancer.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=C225+Cy5%2E5+synthesis)]

The synthesis of C225-Cy5.5 was described by Soukos et al. (11). Both C225 and Cy5.5 were obtained from commercial sources for studies detailed in this chapter. The MAb (formulation not described) was dissolved in 0.1 M bicarbonate buffer (pH 9.3), and a solution of Cy5.5 in the same buffer was added to it. The solution mixture was incubated in the dark for 3 h at room temperature, followed by dialysis three times against excess phosphate buffer (pH 7.4) to remove any unbound dye. For use as controls, bovine serum albumin (BSA)-Cy5.5 and mouse IgG (IgG)-Cy5.5 conjugates were also prepared following the method detailed above. The C225-Cy5.5 and the BSA- and IgG-Cy5.5 conjugates were reported to have 2.1 and 1.6 molecules of Cy5.5, respectively, attached to each protein as determined with a spectroscopic method. The purity, yield, and stability of the various conjugates was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=C225+Cy5%2E5+in+vitro)]

The in vitro binding activity of C225-Cy5.5 was studied with the use of A431 cells, a human epidermoid SCC cell line, and HCPC-1 cells, a cell line derived from an experimentally induced epidermoid carcinoma of the hamster buccal pouch (11). The respective cell lines were grown on glass coverslips and exposed to C225-Cy5.5, BSA-Cy5.5, or mouse IgG-Cy5.5 for 3 h at 37°C. The coverslips were then washed thoroughly with phosphate-buffered saline (pH not reported) and examined under a fluorescence microscope. Both cell lines were reported to show fluorescence only with the C225-Cy5.5 conjugate, indicating that the MAb-Cy5.5 conjugate could be used to detect cell types expressing EGFR under in vitro conditions. No blocking studies with unconjugated C225 were reported.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=C225+Cy5%2E5+rodentia)]

No references are currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=C225+Cy5%2E5+Non+primate+mammals)]

To evaluate the use of C225-Cy5.5 for imaging precancerous lesions in the Syrian golden hamster cheek pouch model, the characteristic premalignancy epithelial changes were induced in the right cheek buccal pouch tissue by painting them with a 5% solution of 7,12-dimethylbenz(a)anthracene (DMBA, a highly potent carcinogen that produces pre-malignancy epithelial changes with increased EGFR expression) in mineral oil 3 times a week for 6 weeks (11). For fluorescent imaging of the premalignant lesions, the hamsters were injected (route of administration not described) with 670 μg of C225-Cy5.5 (n = 9 animals), or 610 μg of IgG-Cy5.5 (n = 6 animals), or 390 μg of BSA-Cy5.5 (n = 6 animals), and imaged from 1 day up to 8 days after the treatment as described by Soukos et al. (11). Although no significant difference in fluorescence intensity ratios (FIR) (fluorescence obtained from DMBA-treated cheek pouch/fluorescence obtained from normal cheek pouch) was noted on day 1 between the animals treated with C225-Cy5.5 (1.17 ± 0.25) and the animals treated with IgG-Cy5.5 (1.01 ± 0.12) or BSA-Cy5.5 (0.95 ± 0.18). By day 6, a significant (P < 0.005) difference was apparent between the MAb-Cy5.5 (FIR was 1.54 ± 0.46) and control animals (FIR was 0.96 ± 0.09 to 0.99 ± 0.01, respectively, for the two groups in the order given above). This indicated that an elevated expression of EGFR in the premalignant tissue resulted in an increased binding of C225-Cy5.5 in the cancerous lesions. No blocking studies were reported.

In an another study, Soukos et al. investigated the use of C225-Cy5.5 to monitor photoimmunotherapy for the treatment of premalignant oral cancer lesions on the hamster cheek pouch with a C225-C_e6_ conjugate, a photosensitizer (11). The premalignant lesions were generated as described above (n = 11 animals), and the cheek pouches (DMBA-treated and normal) of the animals were divided into two equal parts with the outer part designated for exposure to light and the inner part designated for protection from light with a black cloth. The animals were injected with the C225-C_e6_ conjugate, and 2 days later they were exposed to light as described by Soukos et al. (11). To determine efficacy of the photosensitizer conjugate treatment 5 days later, the animals were injected with the C225-Cy5.5 conjugate and fluorescence imaging was performed 3 days after the treatment. A significant difference between the fluorescence of the non–light-exposed areas of the normal and the DMBA-treated cheek pouches was reported (110 ± 21 versus 160 ± 29, P < 0.0005). Under the same experimental conditions, little difference in the fluorescence was observed for the normal cheek pouches with or without light treatment (112 ± 22 versus 110 ± 21). A significant (P < 0.01) difference in the fluorescence of the respective light-exposed (124.2 ± 26) and non–light-exposed DMBA-treated (160 ± 29) cheek areas of the C225-Cy5.5 conjugate injected animals was reported, indicating that the increased expression of EGFR was reduced to normal levels after DMBA treatment because of the photodynamic therapy after injection of the C225-Cy5.5 conjugate. A histological examination of the DMBA-treated cheek pouches confirmed the presence of precancerous lesions in all animals used for the study.

From these studies the investigators concluded that an infrared-emitting fluorophore could be used as an alternative to radioisotope-labeled agents for the detection of premalignant oral cancer lesions. They also concluded that C225-Cy5.5 could possibly be used to monitor oral cancer progression in a preclinical setting.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=C225+Cy5%2E5+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=C225+Cy5%2E5+Human+Studies)]

No references are currently available.

## NIH Support

Some studies mentioned in this chapter were supported by National Institutes of Health grant R01 AR40352.

## References

1 Ke S., Wen X., Gurfinkel M., Charnsangavej C., Wallace S., Sevick-Muraca E.M., Li C. (2003). Near-infrared optical imaging of epidermal growth factor receptor in breast cancer xenografts. Cancer Res.
2 Garcia J., Riely G.J., Nafa K., Ladanyi M. (2008). KRAS mutational testing in the selection of patients for EGFR-targeted therapies. Semin Diagn Pathol.
3 Laurent-Puig P., Lievre A., Blons H. (2009). Mutations and response to epidermal growth factor receptor inhibitors. Clin Cancer Res.
4 Mishani E., Abourbeh G., Eiblmaier M., Anderson C.J. (2008). Imaging of EGFR and EGFR tyrosine kinase overexpression in tumors by nuclear medicine modalities. Curr Pharm Des.
5 Reilly R.M., Kiarash R., Sandhu J., Lee Y.W., Cameron R.G., Hendler A., Vallis K., Gariepy J. (2000). A comparison of EGF and MAb 528 labeled with 111In for imaging human breast cancer. J Nucl Med.
6 Pnwar P., Iznaga-Escobar N., Mishra P., Srivastava V., Sharma R.K., Chandra R., Mishra A.K. (2005). Radiolabeling and biological evaluation of DOTA-Ph-Al derivative conjugated to anti-EGFR antibody ior egf/r3 for targeted tumor imaging and therapy. Cancer Biol Ther.
7 Wygoda Z., Kula D., Bierzynska-Macyszyn G., Larysz D., Jarzab M., Wlaszczuk P., Bazowski P., Wojtacha M., Rudnik A., Stepien T., Kaspera W., Etmanska A., Skladowski K., Tarnawski R., Kokocinska D., Jarzab B. (2006). Use of monoclonal anti-EGFR antibody in the radioimmunotherapy of malignant gliomas in the context of EGFR expression in grade III and IV tumors. Hybridoma (Larchmt).
8 Withrow K.P., Newman J.R., Skipper J.B., Gleysteen J.P., Magnuson J.S., Zinn K., Rosenthal E.L. (2008). Assessment of bevacizumab conjugated to Cy5.5 for detection of head and neck cancer xenografts. Technol Cancer Res Treat.
9 Gleysteen J.P., Newman J.R., Chhieng D., Frost A., Zinn K.R., Rosenthal E.L. (2008). Fluorescent labeled anti-EGFR antibody for identification of regional and distant metastasis in a preclinical xenograft model. Head Neck.
10 Barrett T., Koyama Y., Hama Y., Ravizzini G., Shin I.S., Jang B.S., Paik C.H., Urano Y., Choyke P.L., Kobayashi H. (2007). In vivo diagnosis of epidermal growth factor receptor expression using molecular imaging with a cocktail of optically labeled monoclonal antibodies. Clin Cancer Res.
11 Soukos N.S., Hamblin M.R., Keel S., Fabian R.L., Deutsch T.F., Hasan T. (2001). Epidermal growth factor receptor-targeted immunophotodiagnosis and photoimmunotherapy of oral precancer in vivo. Cancer Res.